# 1-(2-{(2R)-1-[(2-[^18^F]Fluorophenyl)sulfonyl]pyrrolidin-2-yl}ethyl)-4-methylpiperidine

Chemical name: | 1-(2-{(2R)-1-[(2-[^18^F]Fluorophenyl)sulfonyl]pyrrolidin-2-yl}ethyl)-4-methylpiperidine
Abbreviated name: | [^18^F]-2FP3
Synonym:
Agent category: | Compound
Target: | 5-HT_7_ serotonin receptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2FP3%20PET)]

5-Hydroxytryptamine (5-HT), commonly known as serotonin, has diverse physiological roles as a neurotransmitter in the central nervous system (1). 5-HT is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are five receptor subtypes within the G-protein–coupled 5-HT_1_ receptor family: 5-HT_1A_, 5-HT_1B_, 5-HT_1D_, 5-HT_1E_, and 5-HT_1F_.

5-HT_7_ receptors are abundantly present in the hippocampus, thalamus, and hypothalamus; low densities are observed in the cortex and amygdala (5-7). 5-HT_7_ receptors are involved in the mediation of emotion and the function of the hypothalamus. 5-HT_7_ receptors are implicated in anxiety, depression, hallucinogenic behavior, circadian rhythms and sleep, memory, epilepsy, and pain. Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_7_ receptors. 1-(2-{(2R)-1-[(2-[^18^F]Fluorophenyl)sulfonyl]pyrrolidin-2-yl}ethyl)-4-methylpiperidine ([^18^F]-2FP3) was evaluated as a positron emission tomography (PET) probe for 5-HT_7_ receptors because the unlabeled 2FP3 was found to be a selective 5-HT_7_ antagonist with nanomolar affinity for the 5-HT_7_ receptor.

### Related Resource Links:

- Chapters in MICAD (5-HT_7_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT7+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_7_ (http://www.ncbi.nlm.nih.gov/gene/3363))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_7_ (http://omim.org/entry/182137))
- Clinical trials (5-HT (http://www.clinicaltrials.gov/ct2/results?term=5-HT))
- Drug information in Food and Drug Administration (5-HT_7_ (http://google2.fda.gov/search?q=5-HT7&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2FP3%20and%20synthesis)]

The automated radiosynthesis of [^18^F]-2FP3 involved standard fluoronucleophilic substitution of the corresponding nitro precursor with K[^18^F]F/Kryptofix2.2.2 in dimethyl sulfoxide for 10 min at 150°C in an automated radiosynthesis unit, followed by solid-phase extraction with C18 cartridge (8, 9). The reported overall radiochemical yield of the radiosynthesis was 48% at the end of bombardment, with a specific activity of 40–130 MBq/nmol (1.1–3.5 mCi/nmol) at the end of synthesis, and a radiochemical purity of >98%. The total synthesis time was 100–120 min. The log P value for [^18^F]-2FP3 was 1.2–1.4.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2FP3%20and%20in%20vitro)]

Lemoine et al. (8) performed in vitro autoradiography in rat brains with [^18^F]-2FP3, which exhibited radioactivity in the cingulate cortex, hippocampus, cerebellum, and thalamus. The radioactivity in the cortex and hippocampus was inhibited by SB269970 (a selective 5-HT_7_ receptor antagonist), with 43% inhibition at 10 nM and 80% inhibition at 1,000 nM. In vitro binding was performed with CHO cells transfected with human recombinant 5-HT receptors. The binding affinity K_d_ values of [^18^F]-2FP3 for 5-HT_7_ receptors was 1.43 nM with little affinity for 5-HT_1A_ and 5-HT_6_ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2FP3%20and%20rodentia)]

Ex vivo stability studies of [^18^F]-2FP3 in the brains of rats (n = 3/group) were performed at 10, 20, 30, and 40 min after intravenous injection of 55.5 MBq (1.5 mCi) [^18^F]-2FP3. [^18^F]-2FP3 remained >95% intact at these time points as determined with HPLC (8).

Rat brains were excised at 20 min after injection of 55.5 MBq (1.5 mCi) [^18^F]-2FP3. Ex vivo PET imaging studies (n = 3/group) were performed at 45 min after the brains were removed (8). Higher radioactivity levels were observed in the cingulate cortex and hippocampus than in the striatum and cerebellum. Pretreatment with excess SB269970 (30 min, 5 mg/kg) decreased [^18^F]-2FP3 binding in all brain areas.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2FP3%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Lemoine et al. (8) performed in vivo PET imaging studies in the brains of two male cats for 90 min after injection of 74 MBq (2 mCi) [^18^F]-2FP3. High initial radioactivity levels were observed in the cingulate cortex, thalamus, hippocampus, and cerebellum. Pretreatment with excess SB269970 (30 min, 5 mg/kg) decreased [^18^F]-2FP3 binding in these brain areas to background levels.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2FP3%20and%20nonhuman%20primate)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2FP3%20and%20human)]

No publication is currently available.

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Bard J.A., Zgombick J., Adham N., Vaysse P., Branchek T.A., Weinshank R.L. (1993). Cloning of a novel human serotonin receptor (5-HT7) positively linked to adenylate cyclase. J Biol Chem.
6 Varnas K., Thomas D.R., Tupala E., Tiihonen J., Hall H. (2004). Distribution of 5-HT7 receptors in the human brain: a preliminary autoradiographic study using [3H]SB-269970. Neurosci Lett.
7 Martin-Cora F.J., Pazos A. (2004). Autoradiographic distribution of 5-HT7 receptors in the human brain using [3H]mesulergine: comparison to other mammalian species. Br J Pharmacol.
8 Lemoine L., Andries J., Le Bars D., Billard T., Zimmer L. (2011). Comparison of 4 radiolabeled antagonists for serotonin 5-HT(7) receptor neuroimaging: toward the first PET radiotracer. J Nucl Med.
9 Andries J., Lemoine L., Le Bars D., Zimmer L., Billard T. (2011). Synthesis and biological evaluation of potential 5-HT(7) receptor PET radiotracers. Eur J Med Chem.